# Copper 1,4,8,11-tetraazacyclotetradecane-N,N',N'',N'''-tetraacetic acid-octreotide

Chemical name: | Copper 1,4,8,11-tetraazacyclotetradecane-N,N',N'',N'''-tetraacetic acid-octreotide
Abbreviated name: | Cu-TETA-OC; ^64^Cu-TETA-OC; ^64^Cu-TETA-octreotide; ^64^Cu-TETA-OC
Synonym:
Agent Category: | Compound
Target: | Somatostatin receptor
Target Category: | Binding of the octreotide
Method of detection: | PET
Source of signal: | ^64^Cu
Activation: | No
Studies: | - In vitro; - Rodents; - Non-human primates; - Humans

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22copper%201%2C4%2C8%2C11--tetraazacyclotetradecane-N%2C%20N%27%2C%20N%27%27%2C%20N%27%27%27-tetraacetic%20acid-octreotide%22%5BSubstance%20Name%5D)]

Somatostatin is a tetradecapeptide acting as an inhibitor of the release of somatotropin, glucagon, gastrointestinal hormones, and other secretory proteins. The targeting of somatostatin receptors with radiolabeled peptides has led to the development of a variety of agents for both diagnostic imaging and radiotherapy of somatostatin receptor-positive tumors, an area of cancer research where considerable progress has been made over the last few years.

^64^Cu-TETA-octreotide (or ^64^Cu-TETA-OC) is a somatostatin receptor showing high affinity for binding, both in vitro and in vivo (1). Its high rate of lesion detection, favorable dosimetry, and clearance properties make it a promising agent for positron emission tomography (PET) imaging of neuroendocrine tumors in patients (2). ^64^Cu -TETA-OC displays a similar affinity as ^111^In-DTPA-octreotide, a clinically approved imaging agent for somatostatin receptor-positive tumors.

Several animal studies also showed the therapeutic value of ^64^Cu-TETA-OC as a tumor growth inhibitor (3). The mechanism of the tumor cell killing process is still unclear and currently under investigation (4). Preliminary subcellular distribution studies suggest a possible role played by the localization of ^64^Cu to the tumor cell nuclei, a result from the dissociation of the metal from macrocyclic chelators in vivo (5) , followed by trafficking of the radiometal to the cell nuclei (4).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22copper%201%2C4%2C8%2C11--tetraazacyclotetradecane-N%2C%20N%27%2C%20N%27%27%2C%20N%27%27%27-tetraacetic%20acid-octreotide%22%5BSubstance%20Name%5D%20AND%20synthesis%5BAll)]

TETA-OC can be prepared following a procedure by Anderson et al. (3). Briefly, the OC is protected with a tert-butoxycarbonyl (Boc) group by reaction with (Boc)_2_O in Me_2_SO, and TETA·4HCl·4H_2_O is neutralized with 4.5 equivalents of aqueous LiOH. The N-terminal amine of Boc-protected OC is conjugated to one of the carboxylic acid moieties on TETA with HBTU in Me_2_SO, using di-isopropylethylamine and hydroxybenzotriazole as catalysts.

^64^Cu-TETA-OC can be synthesized using the method described by Bass et al. (6). This procedure involves diluting ^64^CuCl_2_ with 0.1 M NH_4_OAc, at pH 5.5, then adding to TETA-OC and adjusting the final volume to 1.0-1.5 ml with buffer. After a 60-min incubation at room temperature, ^64^Cu-TETA-OC is purified using a Sep-Pak cartridge (7). By following this procedure, the radiochemical purity of ^64^Cu-TETA is >90%, and the radiochemical purity of ^64^Cu-TETA-OC is >95% (by high-performance liquid chromatography, HPLC) (8).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22copper%201%2C4%2C8%2C11--tetraazacyclotetradecane-N%2C%20N%27%2C%20N%27%27%2C%20N%27%27%27-tetraacetic%20acid-octreotide%22%5BSubstance%20Name%5D%20AND%20in%20vitro)]

In vitro studies on somatostatin receptor-positive AR42J rat pancreatic tumors and focused on the subcellular distribution of ^64^Cu -TETA-OC showed a localization of substantial quantities of ^64^Cu to the cell nucleus and mitochondria (4). This process was shown to be a main contributing factor in the tumor cell killing process (4). It was also suggested that the instability of the moiety of ^64^Cu-TETA under biological conditions was the cause of the translocation of ^64^Cu to the nucleus.

Wang et al. (4) observed that the majority of ^64^Cu-TETA-OC was internalized in AR42J cells by receptor-mediated endocytosis. This internalization process increased steadily over a 24-h time period, with low amounts of cell surface-associated activity, suggesting a rapid turnover and recycling of SSTR2 receptors.

Using a procedure modified from the one by Zinn et al. (9), Wang et al. (4) showed that the percentage of surface-bound, cell-associated activity ranged from almost 7% to >16%, with the amount of surface-bound activity increasing at 24 h, and that the majority of ^64^Cu-TETA-OC was internalized.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22copper%201%2C4%2C8%2C11--tetraazacyclotetradecane-N%2C%20N%27%2C%20N%27%27%2C%20N%27%27%27-tetraacetic%20acid-octreotide%22%5BSubstance%20Name%5D%20AND%20rodentia%5BMeSH)]

^64^Cu-TETA-OC was shown to inhibit the growth of somatostatin receptor-positive tumors in rats at doses exhibiting minimal toxicity. In one study, Anderson et al. (3) performed experiments on rats bearing palpable CA20948 pancreatic tumors by injecting them with either a single 15-mCi dose, a fractionated amount of 15 mCi given in two to three doses over 2-8 days, or control agents of buffer OC. Results showed that ^64^Cu-TETA-OC could greatly inhibit the growth of pancreatic tumors at doses causing minimal toxicity. The only toxicity observed in treated rats was a decrease in the white blood cell count, a significant drop for rats treated by single injection, and a slight decrease (with rebound) for those receiving a fractionated dose treatment. Injection of fractionated doses appeared to be more effective than a single dose treatment, showing a 25% reduction in tumor growth rate compared with single-dose injections (and a 75% reduction for the buffer control group). Estimated absorbed doses of ^64^Cu-TETA-OC to the tumor were between 465 and 540 rads. At those doses, tumor inhibition—and even tumor regression (for large tumors)—was observed; however, all tumors eventually re-grew.

Using a model of tumor-bearing Lewis rats, the estimated human absorbed doses to normal organs showed the bladder wall (1.12 rad/mCi) and the lower large intestine (0.86 rad/mCi) to be the primary and secondary critical organs; the human effective dose equivalent was found to be 0.21 rad/mCi (3). ^64^Cu-TETA-OC and ^111^In-DTPA-OC showed similar biodistributions in tumor-bearing rat models (7).

Rat studies performed by de Jong et al. (10) showed that altering the OC structure slightly (by substitution of a tyrosine for phenylalanine, for example) resulted in a better uptake of the peptide in receptor-rich tissues such as adrenals, pancreas, pituitary, and tumor. However, rat studies showed retention of the activity of ^64^Cu-TETA-OC in the blood, liver, and bone marrow, suggesting a possible dissociation of ^64^Cu from TETA in vivo. In their study, Bass et al. (6) showed that ^64^Cu dissociated from ^64^Cu-TETA-OC and bound to proteins in large concentrations, such as superoxide dismutase (6).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22copper%201%2C4%2C8%2C11--tetraazacyclotetradecane-N%2C%20N%27%2C%20N%27%27%2C%20N%27%27%27-tetraacetic%20acid-octreotide%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20s)]

No reference currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22copper%201%2C4%2C8%2C11--tetraazacyclotetradecane-N%2C%20N%27%2C%20N%27%27%2C%20N%27%27%27-tetraacetic%20acid-octreotide%22%5BSubstance%20Name%5D%20AND%20%28baboon%20OR%25)]

PET imaging studies using ^64^Cu-TETA-OC have been performed using non-human primates to estimate human absorbed doses. Data obtained by Anderson et al. (2) for ^64^Cu-TETA-OC PET imaging on baboons showed the dose-limiting organs to be the bladder wall (0.62 rad/mCi), followed by the kidneys (0.49 rad/mCi). The estimated human absorbed dose for the total body was found to be 0.07 rad/mCi. The large discrepancy between dosimetry in rats and baboons obtained for the intestinal absorbed doses was explained by the very different excretion patterns of these animals.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22copper%201%2C4%2C8%2C11--tetraazacyclotetradecane-N%2C%20N%27%2C%20N%27%27%2C%20N%27%27%27-tetraacetic%20acid-octreotide%22%5BSubstance%20Name%5D%20AND%20human)]

Human absorbed doses of ^64^Cu-TETA-OC to normal organs were estimated from biodistribution data in both tumor-bearing Lewis rats and baboons (2) (see sections on rodents and non-human primates).

Anderson et al. (2) performed ^64^Cu-TETA-OC PET studies on eight patients with histologically proven neuroendocrine tumors (five with carcinoid tumors of the gastrointestinal tract and three with pancreatic islet cell tumors). Pharmacokinetic analysis of blood samples obtained from patients showed that ^64^Cu-TETA-OC PET cleared rapidly from the blood. However, 7.9 ± 3.7% injected dose (ID) remained (range, 3.2-13.5 %ID) 4 h after injection. The activity decreased further from 6 to 22 h, with amounts ranging from 0.8 to 6.6 %ID (mean, 3.3 ± 2.3%ID). Large variations were observed from patient to patient. Similarly to the results obtained in rat studies, ^64^Cu was retained in the blood, and ^64^Cu-TETA-OC did not completely clear from the circulation (7).

Comparative studies between ^64^Cu-TETA-OC PET and ^111^In-DTPA-OC scintigraphy showed that, in general, more lesions were detected using ^64^Cu-TETA-OC because of the higher resolution obtained with PET imaging. Nevertheless, the image quality was in some cases superior by using DTPA because of the absence of intense activity in the bladder and kidneys when using ^111^In-DTPA-OC (2).

## References

1 Lewis JS, Lewis MR, Srinivasan A, Schmidt MA, Wang J, Anderson CJ. (1999). Comparison of four 64Cu-labeled somatostatin analogues in vitro and in a tumor-bearing rat model: evaluation of new derivatives for positron emission tomography imaging and targeted radiotherapy. J Med Chem.
2 Anderson CJ, Dehdashti F, Cutler PD, Schwarz SW, Laforest R, Bass LA, Lewis JS, McCarthy DW. (2001). 64Cu-TETA-octreotide as a PET imaging agent for patients with neuroendocrine tumors. J Nucl Med.
3 Anderson CJ, Jones LA, Bass LA, Sherman EL, McCarthy DW, Cutler PD, Lanahan MV, Cristel ME, Lewis JS, Schwarz SW. (1998). Radiotherapy, toxicity and dosimetry of copper-64-TETA-octreotide in tumor-bearing rats. J Nucl Med.
4 Wang M, Caruano AL, Lewis MR, Meyer LA, van der Waal RP, Anderson CJ. (2003). Subcellular localization of radiolabeled somatostatin analogues: implications for targeted radiotherapy of cancer. Cancer Res.
5 Fjalling M, Andersson P, Forssell-Aronsson E, Gretarsdottir J, Johansson V, Tisell LE, Wangberg B, Nilsson O, Berg G, Michanek A, Lindstedt G, Ahlman H. (1996). Systemic radionuclide therapy using indium-111-DTPA-D-Phe1-octreotide in midgut carcinoid syndrome. J Nucl Med.
6 Bass LA, Wang M, Welch MJ, Anderson CJ. (2000). In vivo transchelation of copper-64 from TETA-octreotide to superoxide dismutase in rat liver. Bioconjug Chem.
7 Anderson CJ, Pajeau TS, Edwards WB, Sherman EL, Rogers BE, Welch MJ. (1995). In vitro and in vivo evaluation of copper-64-octreotide conjugates. J Nucl Med.
8 Siegel BA, Dehdashti F, Mutch DG, Podoloff DA, Wendt R, Sutton GP, Burt RW, Ellis PR, Mathias CJ, Green MA, Gershenson DM. (2003). Evaluation of 111In-DTPA-folate as a receptor-targeted diagnostic agent for ovarian cancer: initial clinical results. J Nucl Med.
9 Zinn KR, Chaudhuri TR, Buchsbaum DJ, Mountz JM, Rogers BE. (2001). Simultaneous evaluation of dual gene transfer to adherent cells by gamma-ray imaging. Nucl Med Biol.
10 de Jong M, Bakker WH, Breeman WA, Bernard BF, Hofland LJ, Visser TJ, Srinivasan A, Schmidt M, Behe M, Macke HR, Krenning EP. (1998). Pre-clinical comparison of [DTPA0] octreotide, [DTPA0,Tyr3] octreotide and [DOTA0,Tyr3] octreotide as carriers for somatostatin receptor-targeted scintigraphy and radionuclide therapy. Int J Cancer.